# ^67^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-3-{2-[2-(3-amino-propoxy)-ethoxy]-ethoxy}-propylamine-γ-folate

Chemical name: | ^67^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-3-{2-[2-(3-amino-propoxy)-ethoxy]-ethoxy}-propylamine-γ-folate
Abbreviated name: | ^67^Ga-P1254
Synonym:
Agent category: | Compound
Target: | Putative folate receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal: | ^67^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1254)]

Folic acid (folate) is a water-soluble B vitamin (1) that is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through the facilitated transporter, which has a low affinity for folate (Michaelis constant (K_m_) = 1–5 μM). Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a higher-affinity (dissociation constant (K_d_) = 0.5 nM) receptor that allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells have been found to overexpress folate-binding protein (2). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in the corresponding normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the folate receptor but at lower frequencies (20%–50%). Activated macrophages, but not resting macrophages, have been also found to have the folate receptor (3).

Several folate-based conjugates (^111^In-DTPA-folate, ^99m^Tc-EC-folate, and [^18^F]FBA-folate) have been studied in tumor imaging (4-8). Deferoxamine (DF), a chelating agent, was conjugated to folic acid forming a mixture of two isomers, DF-α-folate and DF-γ-folate. Only the DF-γ-folate isomer was able to displace [^3^H]folic acid from its receptors with a 50% inhibition concentration similar to that of folic acid (2.5 nM versus 2.4 nM) (9). ^68/67/66^Ga-γ-DF-folate is being developed as an imaging agent for the detection of folate receptors in vivo with either positron emission tomography or single-photon emission computed tomography. In this chapter, Fani et al. (10) prepared a γ-folate conjugate with tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) and 3-{2-[2-(3-amino-propoxy)-ethoxy]-ethoxy}-propylamine as a spacer to form P1254, which was labeled with ^67^Ga for detection of folate receptors.

### Related Resource Links:

- Chapters in MICAD (folate receptor (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in OMIM (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptors (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (folate receptor (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1254%20and%20synthesis)]

Fani et al. (10) coupled P1254 (10 nmol) with 74 MBq (2 mCi) ^67^GaCl_3_ in acetate buffer (pH 5) for 30 min at 95°C to yield ^67^Ga-P1254 with >95% radiochemical purity. Radiochemical yield was >95% with a specific activity of 7 MBq/nmol (0.19 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1254%20and%20in%20vitro)]

The human nasopharyngeal carcinoma KB cell line has putative folate receptors as determined with ^67^Ga-P1254 saturation binding studies at 4°C (10). ^67^Ga-P1254 showed a K_d_ (affinity constant) of 4.27 ± 0.42 nM and a B_max_ (receptor density) of 11.45 ± 0.27 nM. There were ~6.9 × 10^6^ folate binding sites per KB cell. ^67^Ga-P1254 (2.5 nM) was rapidly associated with KB cells at 37°C with 56% of incubation dose (ID) at 30 min and ~70% ID at 4 h. Approximately 12% ID of ^67^Ga-P1254 was internalized at 4 h. Excess folate blocked the cell-associated radioactivity to <0.5% ID. Approximately 82% of radioactivity was retained in the cells after 4 h incubation in fresh medium.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1254%20and%20rodentia)]

Fani et al. (10) performed ex vivo biodistribution studies of 1.5 MBq (0.041 mCi, 0.4 nmol) ^67^Ga-P1254 in nude mice (n = 4–7/group) bearing KB and HT1080 (low folate receptor expression) tumor xenografts. Accumulation of ^67^Ga-P1254 in the KB tumors was 12.5 ± 1.5, 10.4 ± 0.4, and 13.1 ± 0.7% ID/g at 1, 2, and 4 h after injection, respectively. The accumulation in the HT1080 tumors was 1.3%–2.4% ID/g at these time points. The organ with the highest accumulation at 4 h after injection was the kidney (104.0% ID/g), followed by the adrenal (3.0% ID/g), pancreas (2.8% ID/g), liver (2.2% ID/g), heart (1.9% ID/g), and pituitary (1.7% ID/g). The accumulation in the blood was low (<0.4% ID/g). The tumor/blood ratios were 39, 41, and 63 at 1, 2, and 4 h, respectively. Pretreatment with excess folate (40 nmol, 5 min before injection) reduced the radioactivity accumulation by >90% in the tumors and kidney at 4 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1254%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1254%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1254%20and%20human)]

No publication is currently available.

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Nakashima-Matsushita N., Homma T., Yu S., Matsuda T., Sunahara N., Nakamura T., Tsukano M., Ratnam M., Matsuyama T. (1999). Selective expression of folate receptor beta and its possible role in methotrexate transport in synovial macrophages from patients with rheumatoid arthritis. Arthritis Rheum.
4 Mathias C.J., Hubers D., Low P.S., Green M.A. (2000). Synthesis of [(99m)Tc]DTPA-folate and its evaluation as a folate-receptor-targeted radiopharmaceutical. Bioconjug Chem.
5 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
6 Mathias C.J., Wang S., Low P.S., Waters D.J., Green M.A. (1999). Receptor-mediated targeting of 67Ga-deferoxamine-folate to folate-receptor-positive human KB tumor xenografts. Nucl Med Biol.
7 Mathias C.J., Wang S., Waters D.J., Turek J.J., Low P.S., Green M.A. (1998). Indium-111-DTPA-folate as a potential folate-receptor-targeted radiopharmaceutical. J Nucl Med.
8 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and Preclinical Evaluation of a Folic Acid Derivative Labeled with 18F for PET Imaging of Folate Receptor-Positive Tumors. J Nucl Med.
9 Wang S., Lee R.J., Mathias C.J., Green M.A., Low P.S. (1996). Synthesis, purification, and tumor cell uptake of 67Ga-deferoxamine--folate, a potential radiopharmaceutical for tumor imaging. Bioconjug Chem.
10 Fani M., Wang X., Nicolas G., Medina C., Raynal I., Port M., Maecke H.R. (2011). Development of new folate-based PET radiotracers: preclinical evaluation of Ga-DOTA-folate conjugates. Eur J Nucl Med Mol Imaging.